# Cy5.5-Human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion protein

Chemical name: | Cy5.5-Human serum albumin-tissue inhibitor of matrix metalloproteinase 2 fusion protein
Abbreviated name: | Cy5.5-HSA/TIMP-2
Synonym: | Cy5.5-HSA-TIMP2, Cy5.5-HSA-TIMP-2
Agent category: | Protein
Target: | α_3_β_1_ integrin
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence
Source of signal/contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure is currently not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). There are four members of endogenous tissue inhibitors of metalloproteinases (TIMPs), which regulate the activity of MMPs leading to inhibition of tumor growth and metastasis (9, 10). TIMP-2 (TIMP2) is a bifunctional inhibitor of angiogenesis that inhibits the proteinase activity of MMPs and endothelial cell proliferation via binding to α_3_β_1_ (the N-terminal domain) and MMP-independent anti-angiogenic activity (the C-terminal domain) (11, 12). Kang et al. (13) fused the N-terminal domain of TIMP2 to the C-terminus of human serum albumin (HSA) to form HSA/TIMP-2 (HSA-TIMP2) fusion protein, which is readily secreted by the transfected yeast Saccharomyces cerevisiae. HSA/TIMP2 retains its anti-angiogenic activity at the C-terminal domain with little MMP inhibitory activity at the N-terminal domain. Lee et al. (14) evaluated Cy5.5-HSA/TIMP-2 (Cy5.5-HSA-TIMP2) for in vivo near-infrared (NIR) fluorescence imaging of rat prostate MLL tumors in nude mice, which showed maximum tumor accumulation at 2 d after injection.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D), TIMP (http://www.ncbi.nlm.nih.gov/books?term=TIMP%20AND%20micad%5Bbook%5D), RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (TIMP2 (http://www.ncbi.nlm.nih.gov/gene/7077), HSA (http://www.ncbi.nlm.nih.gov/gene/213), α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), α_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3675), β_1_ integrin (http://www.ncbi.nlm.nih.gov/gene/3688), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (TIMP2 (http://omim.org/entry/188825), HSA (http://omim.org/entry/103600), α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), α_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/605025), β_1_ integrin (http://www.ncbi.nlm.nih.gov/omim/135630), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (TIMP (http://www.clinicaltrials.gov/ct2/results?term=TIMP), RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (TIMP (http://google2.fda.gov/search?q=TIMP&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*), RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2)]

A solution of Cy5.5-N-hydroxysuccinimide (NHS) ester and HSA-TIMP2 (2:1 molar ratio) was incubated for 1 h at 25°C (14). The NHS ester of Cy5.5 reacted with the α-amino group of the Lys residue of the protein. Unreacted Cy5.5 dye molecules were removed with dialysis. Sodium dodecyl sulfate-polyacrylamide gel electrophoresis (SDS-PAGE) analysis confirmed conjugation of Cy5.5 to the HSA-TIMP2 molecule. The number of Cy5.5 molecules per protein was not reported. Cy5.5-HSA-TIMP2 exhibits a molecular weight of ~88 kDa. Fluorescence excitation and emission maxima of Cy5.5 are 675 nm and 695 nm, respectively.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20in%20vitro)]

Kang et al. (13) showed that 170 µM HSA-TIMP2 exhibited 37% inhibition of MMP-2 activity, whereas 7.5 nM TIMP2 exhibited 50% inhibition. On the other hand, 187 µM HSA-TIMP2 inhibited the capillary-like tube formation (marker of angiogenic activity) of human umbilical vein endothelial cells by 81%. Lee et al. (14) showed that 10 µM Cy5.5-HSA-TIMP2 was able to inhibit the tube formation, indicating that Cy5.5-HSA-TIMP2 retains anti-angiogenic activity.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20rodentia)]

Lee et al. (14) performed in vivo optical imaging studies of Cy5.5-HSA-TIMP2 (200 ng/g body weight) in nude mice (n = 4) bearing rat prostate MLL tumors. Whole-body optical imaging was performed for 7 d after intraperitoneal injection. Good fluorescence signal was visualized in MLL tumors at 1 d, and the signal reached a maximum at 2 d with a gradual decline thereafter. The tumor fluorescence intensities were 9, 10, and 4 × 10^10^ photons/s at 1, 2, and 4 d after injection, respectively. Injection of Cy5.5 in tumor-bearing nude mice (n = 4) showed little fluorescence signal (< 2 × 10^10^ photons/s) in the tumors at 1–7 d after injection. The amount of Cy5.5-HSA-TIMP2 in the tumors was calculated to be 2.25 ± 0.25% of the injected dose at 2 d after injection. Cy5.5-HSA-TIMP2 exhibited a blood half-life of 19.6 ± 3.2 h, whereas Cy5.5 exhibited a blood half-life of 2.2 ± 0.7 h. Ex vivo optical imaging of the excised tissues showed that the tumors exhibited the highest signal, followed by the liver, spleen, stomach, lung, kidney, intestine, heart, muscle, and blood. Confocal microscopy of tumor tissue sections at 2 d and 4 d after injection revealed the Cy5.5 signal within the cells. No blocking studies were performed. The investigators suggested that tumor accumulation of Cy5.5-HSA-TIMP2 may be due to the effects of enhanced permeability/retention and tumor uptake of albumin in addition to its anti-angiogenic activity on the tumor endothelial cells.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=HSA-TIMP-2%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Baker A.H., Edwards D.R., Murphy G. (2002). Metalloproteinase inhibitors: biological actions and therapeutic opportunities. J Cell Sci.
10 Jiang Y., Goldberg I.D., Shi Y.E. (2002). Complex roles of tissue inhibitors of metalloproteinases in cancer. Oncogene.
11 Fernandez C.A., Butterfield C., Jackson G., Moses M.A. (2003). Structural and functional uncoupling of the enzymatic and angiogenic inhibitory activities of tissue inhibitor of metalloproteinase-2 (TIMP-2): loop 6 is a novel angiogenesis inhibitor. J Biol Chem.
12 Seo D.W., Li H., Guedez L., Wingfield P.T., Diaz T., Salloum R., Wei B.Y., Stetler-Stevenson W.G. (2003). TIMP-2 mediated inhibition of angiogenesis: an MMP-independent mechanism. Cell.
13 Kang W.K., Park E.K., Lee H.S., Park B.Y., Chang J.Y., Kim M.Y., Kang H.A., Kim J.Y. (2007). A biologically active angiogenesis inhibitor, human serum albumin-TIMP-2 fusion protein, secreted from Saccharomyces cerevisiae. Protein Expr Purif.
14 Lee M.S., Kim Y.H., Kim Y.J., Kwon S.H., Bang J.K., Lee S.M., Song Y.S., Hahm D.H., Shim I., Han D., Her S. (2011). Pharmacokinetics and biodistribution of human serum albumin-TIMP-2 fusion protein using near-infrared optical imaging. J Pharm Pharm Sci.